# Radioiodinated anti-TAG-72 CC49 tetravalent single-chain Fv antibody

Chemical name: | Radioiodinated anti-TAG-72 CC49 tetravalent single-chain Fv antibody
Abbreviated name: | ^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ Ab
Synonym: | ^125^I/^131^I-CC49 Ab, ^125^I/^131^I-CC49 tetravalent single-chain Fv recombinant antibody, ^125^I/^131^I-tetrameric CC49 [sc(Fv)_2_]_2_
Agent Category: | Tetravalent single-chain Fv antibody construct ([sc(Fv)_2_]_2_ Ab)
Target: | TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission tomography (SPECT). planar gamma imaging
Source of signal: | ^125^I, ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(single-chain+antibody+construct+of+MAb+CC49)+OR+(tetravalent+single-chain+Fv+CC49))]

Radioiodinated Anti-TAG-72 CC49 tetravalent single-chain Fv antibody (^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ Ab), which is formed by the conjugation of ^125^I or ^131^I with a bioengineered recombinant anti–tumor-associated glycoprotein 72 (TAG-72) antibody construct, has been developed for gamma imaging of cancers that express TAG-72 (1, 2). ^125^I has a physical half-life (t_½_) of 60 days with a gamma energy that is not ideal for in vivo imaging. ^131^I has a physical half-life (t_½_) of 8.02 days with a gamma energy that is high but acceptable for in vivo imaging.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (3-6). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (7). The murine monoclonal antibody (MAb) B72.3 against TAG-72 was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (8). With the use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-72 MAbs with higher affinity constants (K_a_) have been produced and characterized (3, 4, 8, 9).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (10). Radiolabeled B72.3 and CC49 have shown excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (11, 12). Because of their relatively large size, radiolabeled intact MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (9, 13-15). One approach to minimize these problems is reducing intact antibodies to antibody fragments such as F(ab’)_2_ and Fab’ (16). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (9, 17, 18). These scFv constructs contain the variable regions of the light chain (V_L_) and heavy chain (V_H_) connected by a flexible linker. Colcher et al. (19) constructed the monomeric CC49 scFv Ab (~27 kDa), which selectively recognizes a unique sialyl-Tn epitope of TAG-72. The radioiodinated CC49 scFv appeared to clear rapidly from the blood with good tumor penetration (18, 20). To further improve the imaging kinetics, Pavlinkova et al. (20) constructed the high-affinity dimer CC49 sc(Fv)_2_ (~60 kDa). The radioiodinated CC49 sc(Fv)_2_ showed good stability and increased avidity in vivo compared with the radioiodinated CC49 scFv construct. Goel et al. (1) formed the tetravalent [sc(Fv)_2_]_2_ construct (~120 kDa) that exhibited four potentially active antigen-binding sites and showed improved in vitro binding properties. Radioiodinated CC49 [sc(Fv)_2_]_2_ (^125^I/^131^I-CC49 [sc(Fv)_2_]_2_) was studied and evaluated for potential cancer therapy and diagnosis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(tetravalent+single-chain+Fv+CC49))+AND+synthesis)]

Goel et al. (1) and Wittel et al. (2) reported the construction and radiolabeling of the ^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ Ab. The CC49 scFv (V_L_-linker-V_H_) was derived from the murine MAb CC49 cloned in the yeast expression vector pPICZαA and constructed with the 205C linker with 25 amino acids (LSADDAKKDAAKKDDAKKDDAKKDL). The bacterial scFv construct was used as the template DNA for the expression of the scFv in competent methylotrophic Pichia pastoris KM71 cells. The construction of the divalent sc(Fv)_2_ (V_L_-linker-V_H_-linker-V_L_-linker-V_H_-His_6_) was performed as described by Goel et al. (21) using the 205C helical linker in a P. pastoris expression system. Upon expression as a protein secreted by P. pastoris, 20–30% of the divalent form was found to spontaneously associate through noncovalent interactions into tetravalent [sc(Fv)_2_]_2_ or higher aggregates (>200 kDa) (1). Purification of scFv was expedited by the use of a hexahistidine tag attached to the COOH-terminal of the construct. The construct was purified from the secreted medium with immobilized metal-affinity chromatography, and the [sc(Fv)_2_]_2_ was separated on a Superdex 200 column. The yield was reported to be 2.0–3.5 mg/L. The preparation was shown to be >95% pure by sodium dodecylsulfate–polyacrylamide gel electrophoresis (SDS-PAGE). The SDS-PAGE study also confirmed that the two polypeptide chains of the tetramer were noncovalently linked. Size-exclusion high-performance liquid chromatography (HPLC) showed the molecular mass to be 120 kDa (9).

Radioiodination of CC49 [sc(Fv)_2_]_2_ Ab was performed with the use of 1,3,4,6-tetrachloro-3α,6α-diphenylglycoluril (IodoGen) as the oxidizing agent (1). Briefly, 20–100 μg of CC49 [sc(Fv)_2_]_2_ Ab in sodium phosphate buffer (pH 7.2) was added to a glass tube coated with IodoGen. Approximately 0.5–1 mCi ^125^I- or ^131^I-labeled sodium iodide was added and the mixture was incubated for 3 min at room temperature (2). Free radioactive iodine was removed by a Sephadex 25 column. Instant thin-layer chromatography or gel filtration HPLC was used to determine the radiochemical purity of the radiolabeled antibody. Goel et al. (1) reported the specific activity of ^125^I- or ^131^I-CC49 [sc(Fv)_2_]_2_ Ab was ~111–333 MBq/mg (3–9 mCi/mg) or 13.3–40.0 MBq/nmol (0.36–1.1 mCi/nmol) on the basis of the molecular mass of 120 kDa. Wittel et al (2) reported that the specific activity of ^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ Ab was only 29.6 MBq/mg (0.8 mCi/mg). The SDS-PAGE showed a radiochemical purity of ≥95%. The size-exclusion HPLC profiles were not altered by the radioiodination procedure.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(tetravalent+single-chain+Fv+CC49))+AND+in+vitro)]

The immunoreactivity of CC49 [sc(Fv)_2_]_2_ Ab was assessed by solid-phase competition enzyme-linked immunosorbent assay (ELISA) and radioimmunoassay using bovine submaxillary gland mucin as the antigen (1, 2). The specific binding for CC49 [sc(Fv)_2_]_2_ Ab was 85–95%, and the nonspecific binding was 0.8–1.5%. Using the surface plasmon resonance technique to measure the real-time interactions, Goel et al. (1) reported the association constant (K_a_) of unlabeled CC49 [sc(Fv)_2_]_2_ to be 1.02 × 10^8^ M−^1^. In comparison, the K_a_ for the intact CC49 MAb and CC49 sc(Fv)_2_ constructs were 1.14 × 10^8^ M−^1^ and 2.75 × 10^7^ M−^1^, respectively. Wittel et al. (2) evaluated [sc(Fv)_2_]_2_ by the solid-phase competitive enzyme-linked immunosorbent assay with the binding of biotinylated CC49 IgG. The [sc(Fv)_2_]_2_ antibody construct was able to inhibit 50% (IC_50_) of the CC49 IgG binding at the concentration of 5.65 x 10−^8^ M. In comparison, the IC_50_ of the whole intact CC40 IgG was 5.0 x 10−^9^ M,

In vitro stability studies of ^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ Ab were conducted by incubating the radiolabeled MAb construct in 1% bovine serum albumin at 37ºC (1). By HPLC analysis, the ^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ MAb was stable in vitro up to 3 days at 37ºC, with ≥90% radioactivity associated with the antibody until 24 h. By 72 h, there was 5.6% radioactivity associated with the smaller sc(Fv)_2_ and 2.9% radioactivity associated with low molecular weight proteins (M_r_ = 45,000 and 30,000). Goel et al. (1) also reported that the unlabeled antibody could be stored at −70ºC for 6 months without any loss of immunoreactivity or evidence of breakdown products.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(tetravalent+single-chain+Fv+CC49))+AND+rodentia)]

Biodistribution studies of ^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ Ab were performed in nude mice bearing s.c. LS-174T human colon carcinomas (~200–300 mm^3^) (1). Dual-label biodistribution studies were conducted with simultaneous i.v. administration of 0.185 MBq (5 μCi) ^125^I-CC49 sc(Fv)_2_ Ab and 0.0925 MBq (2.5 μCi) ^131^I-CC49 [sc(Fv)_2_]_2_ Ab in one group (n = 6) of mice. Another group of mice (n = 6) received 0.185 MBq (5 μCi) ^125^I-CC49 [sc(Fv)_2_]_2_ Ab and 0.0925 MBq (2.5 μCi) ^131^I-CC49 IgG Ab. The elimination half-life (t_½_) of radioiodinated CC49 [sc(Fv)_2_]_2_ Ab was 170 min. The blood clearance had an α-phase and a β-phase. Wittel et al. (2) determined the t_½β_ to be 116.30 min. Goel et al. (1) also found a third phase that corresponded to the clearance of free radioiodine. The whole-body clearance t_½_ was 8.9 ± 1.3 h. At 48 h, ~95% of the radioactivity was cleared from the body. In comparison, only 75% of CC49 IgG radioactivity was cleared in 48 h. There was also a 2-fold increase in the blood biological t_½_ of radioiodinated CC49 [sc(Fv)_2_]_2_ Ab as compared with the dimeric CC49 sc(Fv)_2_. The tumor radioactivity levels of radioiodinated CC49 [sc(Fv)_2_]_2_ Ab in percent injected dose per gram (% ID/g) were 6.2 ± 1.0 (0.5 h), 9.0 ± 1.2 (1 h), 12.3 ± 1.6 (4 h), 21.3 ± 1.3 (6 h), 17.0 ± 1.6 (16 h), 10.5 ± 1.1 (24 h), and 8.2 ± 0.1 (48 h) (1). However, Wittel et al. (2) reported only ~2-7% ID/g tumor radioactivity levels (extrapolated from Figure 3) from 0.5-48 h for the dose of 0.185 MBq (5 μCi) ^125^I-CC49 [sc(Fv)_2_]_2_ Ab. In the study of Goel et al. (1), the radioactivity levels of ^125^I-CC49 sc(Fv)_2_ and ^131^I-CC49 IgG Ab at 6 h were 9.8 ± 1.3% ID/g and 17.3 ± 1.1, respectively. There were also significant radioactivity levels of radioiodinated CC49 [sc(Fv)_2_]_2_ Ab in the spleen, liver, and kidneys. The radioactivity levels (% ID/g) for major organs at 0.5 h were 22.0 ± 0.6 (blood), 7.9 ± 0.6 (liver), 9.0 ± 1.4 (spleen), 8.5 ± 0.6 (kidneys), 4.7 ± 0.3 (heart), and 5.6 ± 0.1 (lungs). At 6 h, these levels changed to 4.5 ± 0.4 (blood), 4.9 ± 0.6 (liver), 5.1 ± 1.5 (spleen), 2.9 ± 0.2 (kidneys), 1.7 ± 0.1 (heart), and 0.7 ± 0.2 (lungs). The tumor/liver, tumor/blood, and tumor/spleen ratios at 24 h were 6.2:1, 35:1, and 10.5:1, respectively.

The in vivo stability of radioiodinated CC49 [sc(Fv)_2_]_2_ Ab in blood plasma was also analyzed with HPLC (1). The ^125^I/^131^I-CC49 [sc(Fv)_2_]_2_ Ab fraction of the radioactivity was >70% at 1 h but only 49% at 2 h. There was 38% radioactivity at 2 h in higher molecular weight forms. Wittel et al. (2) reported that radioiodinatedI-CC49 [sc(Fv)_2_]_2_ Ab remained intact with 60.27% at 1 h, 61.84% at 2 h, and 38.75% at 12 h. The amounts of the higher molecular weight forms (>200 kDa aggregates) were 18.65% at 1 h, 20.78% at 2 h, and 20.00% at 12 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(tetravalent+single-chain+Fv+CC49))++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(tetravalent+single-chain+Fv+CC49))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(tetravalent+single-chain+Fv+CC49))+AND+human)]

No publication is currently available.

## References

1 Goel A., Colcher D., Baranowska-Kortylewicz J., Augustine S., Booth B.J., Pavlinkova G., Batra S.K. (2000). Genetically engineered tetravalent single-chain Fv of the pancarcinoma monoclonal antibody CC49: improved biodistribution and potential for therapeutic application. Cancer Res.
2 Wittel U.A., Jain M., Goel A., Chauhan S.C., Colcher D., Batra S.K. (2005). The in vivo characteristics of genetically engineered divalent and tetravalent single-chain antibody constructs. Nucl Med Biol.
3 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
4 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
5 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
6 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
7 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
8 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
9 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
10 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
11 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
12 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
13 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
14 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
15 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
16 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
17 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
18 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
19 Colcher D., Goel A., Pavlinkova G., Beresford G., Booth B., Batra S.K. (1999). Effects of genetic engineering on the pharmacokinetics of antibodies. Q J Nucl Med.
20 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.
21 Goel A., Beresford G.W., Colcher D., Pavlinkova G., Booth B.J., Baranowska-Kortylewicz J., Batra S.K. (2000). Divalent forms of CC49 single-chain antibody constructs in Pichia pastoris: expression, purification, and characterization. J Biochem (Tokyo).